# ^111^In-Labeled anti-epidermal growth factor receptor human monoclonal antibody 048-006

Chemical name: | ^111^In-Labeled anti-epidermal growth factor receptor human monoclonal antibody 048-006
Abbreviated name: | [^111^In]-048-006
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epidermal%20growth%20factor%20receptor&cmd=DetailsSearch)]

The epidermal growth factor receptor (EGFR) belongs to the ErbB oncogene family and has four subtypes: EGFR (also known as EGFR1), EGFR2, EGFR3, and EGFR4 (1). These receptors mediate their activity through a tyrosine kinase signal transduction pathway (the mechanism of action of the different EGFR receptors is described in brief by Pedersen et al. (2)), are known to promote the proliferation and differentiation of cells, and are involved in the development of several different types of cancers in humans (3). Because EGFR1 is overexpressed in colorectal and head and neck cancers, it is targeted in the clinic with monoclonal antibodies (mAbs) such as cetuximab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=8bc6397e-4bd8-4d37-a007-a327e4da34d9) (a human/mouse chimeric mAb) or panitumumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=e0fa4bca-f245-4d92-ae29-b0c630a315c2) (a recombinant human mAb) for the treatment of these neoplasms. However, these mAbs cannot be used to treat cancers that bear a mutant KRAS oncogene because this gene is constitutively active and is regulated independently of the EGFR. In addition, immunohistochemical analysis of human tumors that did not harbor a KRAS mutation showed that the efficacy of cetuximab does not always correlate with the level of EGFR expression in the cancerous tissues (4). Also, this technique cannot be used to predict the therapeutic outcome for a patient (5). Therefore, it is important to develop a method that can be used to screen, evaluate, and select patients who can benefit most from the anti-EGFR therapy.

Nine human mAb clones that targeted the EGFR were isolated from a phage-display mAb library with an organic solvent method (6). One of the clones, 048-006, was reported to exhibit an in vivo anti-tumor activity against A431 cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology) xenograft tumors in mice that was comparable to cetuximab. In an effort to develop an imaging agent that can be used to screen for patients who would benefit most from cetuximab (or panitumumab) immunotherapy, the in vitro characteristics of 048-006 were studied with human cell lines, and the biodistribution of ^111^In-labeled 048-006 ([^111^In]-048-006) was investigated in nude mice bearing xenograft tumors that expressed different levels of EGFR (5).

### Related Resource Links

EGFR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books?term=EGFR%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=HER2) and protein (http://www.ncbi.nlm.nih.gov/protein?term=HER2) sequences of HER2

EGFR-related clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR) in ClinicalTrials.gov

HER2-related clinical trials (http://clinicaltrials.gov/ct2/results?term=human+epidermal+growth+factor+receptor+type+2+%28HER2%29) in ClinicalTrials.gov

Bioassays of EGFR (http://www.ncbi.nlm.nih.gov/pcassay?term=EGFR) in PubChem BioAssay

EGFR (http://omim.org/entry/131550) in Online Mendelian Inheritance in Man Database (OMIM)

Human EGFR signaling pathway (http://www.genome.jp/kegg-bin/show_pathway?hsa04012) in Kyoto Encyclopedia of genes and Genomes database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D048-006%20synthesis&cmd=DetailsSearch)]

The 048-006 mAb was produced and purified as described elsewhere (5). For in vitro studies, the mAb was directly labeled with ^125^I using the chloramine-T method (5). The radiochemical yield (RCY), radiochemical purity (RCP), specific activity (SA), and stability of the radioiodinated mAbs were not reported.

048-006 was conjugated with [(R)-2-amino-3-(p-isothiocyanato-phenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-N,N,N',N'',N''-pentaacetic acid (p-SCN-Bz-CHX-A'-DTPA) and labeled with ^111^In as described by Sogawa et al. (5). Approximately two molecules of DTPA were reported to be conjugated to each molecule of 048-006 as determined with cellulose acetate electrophoresis. The RCY, RCP, SA, and stability of [^111^In]-048-006 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D048-006%20in%20vitro&cmd=DetailsSearch)]

For use in cell-binding studies, the expression level of EGFR in A4 cells (controls), A431 cells, Hep-G2 cells, SK-Hep1 cells, and HuH-7 cells was investigated with Western blot analysis (5). Compared with the A431 cells (expression level of EGFR in these cells was considered to be 100%), the expression of EGFR in HuH-7 cells, SK-Hep1 cells, Hep-G2 cells, and the A4 cells was 13.83%, 8.32%, 0.02%, and 0.00%, respectively. The amount of EGFR expressed in the xenograft tumors generated from the different cell lines was confirmed with commercially available immunohistochemical staining kit that targeted the receptor. With this technique, no difference was observed in the level of EGFR expressed in tumors produced with the A341 cells and the HuH-7 cells, but the SK-Hep1 cell tumors had a lower level of EGFR compared with the A431 or the HuH-7 cells. The investigators reported that the Hep-G2 cells did not produce any tumors in the mice and were not used in any further studies (5).

The binding of [^125^I]-048-006 and [^111^In]-048-006 was investigated with A431 cells, SK-Hep1 cells, and HuH-7 cells (5). This study showed that the amount of [^111^In]-048-006 that bound to the different types of cells was 83.8 ± 1.1%, 57.2 ± 1.6%, and 49.2 ± 3.2%, respectively; for [^125^I]-048-006, the binding was 81.7 ± 0.2%, 54.6 ± 0.6%, and 58.4 ± 0.2%, respectively. The immunoreactive fractions of [^111^In]-048-006 and [^125^I]-048-006 with the different cell lines were determined to vary from 70.5% to 100% and from 67.2% to 87.4%, respectively (5). The affinity constants of [^111^In]-048-006 and [^125^I]-048-006 with the A431 cells were 2.3 × 10^9^ L/mol and 1.8 × 10^9^ L/mol, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D048-006%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-048-006 was investigated in nude mice bearing A431 cell, HuH-7 cell, SK-Hep1 cell, and A4 cell (control) tumors as detailed by Sogawa et al. (5). The animals (n = 5 animals/time point per cell line) were intravenously administered 37 kBq (1 μCi; 3.33 pmol) of the labeled mAb and euthanized at 1, 2, and 4 d postinjection (p.i.) to retrieve all the organs of interest, including tumors, and to determine the amount of radioactivity accumulated in the various tissues. All results were presented as percent of injected dose per gram tissue (% ID/g) (Table 1).

Table 1: Amount of radioactivity from [ ^ 111 ^ In]-048-006 accumulated in various organs and tumors of mice at different time points.

Organ/Tumor | Accumulated radioactivity (% ID/g)
Organ/Tumor | 1 d p.i. | 2 d p.i. | 4 d p.i.
Blood | 9.6 ± 1.6 | 8.0 ± 1.6 | 4.1 ± 1.6
Liver | 5.4 ± 1.7 | 7.0 ± 1.6 | 6.4 ± 1.8
Spleen | 12.8 ± 2.4 | 9.6 ± 2.9 | 7.1 ± 1.4
Kidney | 13.4 ± 0.7 | 11.5 ± 1.5 | 7.8 ± 1.4
Muscle | 1.2 ± 0.1 | 1.1 ± 0.1 | 0.7 ± 0.2
Tumor (A431 cells) | 12.5 ± 2.6^a^ | 16.0 ± 3.6^b^ | 13.2 ± 3.4^b^
Tumor (HuH-7 cells) | 9.8 ± 2.3 | 21.2 ± 5.8^b,c^ | 16.5 ± 1.3^b,d^
Tumor (SK-Hep1 cells) | 9.4 ± 1.4 | 11.5 ± 1.4^b^ | 8.6 ± 1.5^b^
Tumor (A4 cells) | 8.0 ± 3.0 | 5.3 ± 0.6 | 2.4 ± 1.2

Because the data obtained from mice bearing the four types of tumors were almost similar the normal organ, data presented in this Table are from mice bearing HuH-7 cell or A4 cell tumors. a: P < 0.05 (versus A4); b: P < 0.01 (versus A4); c: P < 0.05 (versus SK-Hep1); and d: P < 0.01 (versus SK-Hep1).

For complete data see ( 5 ).

The amount of tracer in the blood was 9.6 ± 1.6% ID/g at 1 d p.i. and decreased to 4.1 ± 1.6 by 4 d p.i. The uptake of radioactivity in the spleen and the kidneys was high at 1 d p.i. and decreased gradually up to 4 d p.i. The accumulation of label in the liver was the highest at 2 d p.i. (7.0 ± 1.6% ID/g). In general, the three EGFR-positive tumors showed an increase in uptake of radioactivity from 1 d p.i. to 2 d p.i., followed by a decrease at 4 d p.i. At 1 d p.i., the uptake of label in the A431 cell tumors was higher (12.5 ± 2.6% ID/g) than in the HuH-7 cell or the SK-Hep1 cell tumors; however, at 2 d p.i. and 4 d p.i., the accumulation of tracer in the HuH-7 cell tumors was higher (21.2 ± 5.8% ID/g and 16.5 ± 1.3%ID/g, respectively) than in the A341 cell or the SK-Hep1 cell tumors. Among the three tumor types, the SK-Hep1 cell tumors showed the lowest accumulation of radioactivity at all of the time points. The A4 cell tumors (controls) showed a gradual decrease in the uptake of label from 1 d p.i. (8.0 ± 3.0% ID/g) to 4 d p.i. (2.4 ± 1.2% ID/g). At 1 d p.i., the tumor/muscle ratios for the A431 cell, HuH-7 cell, SK-Hep1 cell, or A4 cell (control) tumors were approximately 13, 10, 9 and 8, respectively. No blocking studies were reported.

For gamma planar imaging, mice bearing A431 cell, HuH-7 cell, and A4 cell tumors (number of animals not reported) were given an intravenous injection of 1.83 MBq (67.7 μCi) [^111^In]-048-006, and images were acquired from the rodents (under anesthesia) at 1 d p.i., 2 d p.i., and 4 d p.i (5). The images showed that the A431 cell and the HuH-7 cell tumors were clearly visible at 1 d p.i., and there was an increased accumulation of the tracer in these lesions up to 4 d p.i. The uptake of radioactivity in the A4 cell tumors was undetectable even at 4 d p.i (5).

From these studies, the investigators concluded that [^111^In]-048-006 was suitable for the detection of tumors that express EGFR in mice (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D048-006%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D048-006%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D048-006%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Nedergaard M.K., Hedegaard C.J., Poulsen H.S. (2012). Targeting the epidermal growth factor receptor in solid tumor malignancies. BioDrugs.
2 Pedersen N.M., Breen K., Rodland M.S., Haslekas C., Stang E., Madshus I.H. (2009). Expression of epidermal growth factor receptor or ErbB3 facilitates geldanamycin-induced down-regulation of ErbB2. Mol Cancer Res.
3 Scott A.M., Wolchok J.D., Old L.J. (2012). Antibody therapy of cancer. Nat Rev Cancer.
4 Nunn A.D. (2007). Molecular imaging and personalized medicine: an uncertain future. Cancer Biother Radiopharm.
5 Sogawa C., Tsuji A.B., Yoshida C., Inubushi M., Furukawa T., Koizumi M., Akahori Y., Ukai Y., Kurosawa G., Kurosawa Y., Saga T. (2012). Novel human monoclonal antibody against epidermal growth factor receptor as an imaging probe for hepatocellular carcinoma. Nucl Med Commun.
6 Kurosawa G., Akahori Y., Morita M., Sumitomo M., Sato N., Muramatsu C., Eguchi K., Matsuda K., Takasaki A., Tanaka M., Iba Y., Hamada-Tsutsumi S., Ukai Y., Shiraishi M., Suzuki K., Kurosawa M., Fujiyama S., Takahashi N., Kato R., Mizoguchi Y., Shamoto M., Tsuda H., Sugiura M., Hattori Y., Miyakawa S., Shiroki R., Hoshinaga K., Hayashi N., Sugioka A., Kurosawa Y. (2008). Comprehensive screening for antigens overexpressed on carcinomas via isolation of human mAbs that may be therapeutic. Proc Natl Acad Sci U S A.